# [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a tri-(histidine-glutamate) peptide tag (HE)_3_ on the N-terminal

Chemical name: | [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a tri-(histidine-glutamate) tag (HE)_3_ on the N-terminal
Abbreviated name: | [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_
Synonym:
Agent Category: | Affibody (antibody)
Target: | Epidermal growth factor receptor (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody%20zher2%20342&cmd=DetailsSearch)]

Overexpression of the epidermal growth factor receptor type 2 (HER2) is a characteristic feature of a variety of cancers, and HER2 levels in tumors (primary or metastatic) are often used to screen for patients who would benefit from anti-HER2 antibody (Ab) therapy (e.g., for breast cancer), to determine the efficacy of a treatment regimen, or to predict the prognostic outcome for a patient (1). Single-photon emission computed tomography (SPECT) or gamma planar imaging with ^99m^Tc-labeled ligands that target HER2 are often used to detect, diagnose, and develop a treatment regimen for cancers that overexpress this receptor (2). Although many Abs (monoclonal, recombinant, etc.) and their derivatives (single-chain and monovalent or divalent Fab fragments, etc.) have been developed and approved for clinical use for the imaging or radioimmunotherapy of such cancers, these agents have limited efficacy because of their immunogenicity (development of Abs against the anti-HER2 Abs), pharmacokinetic properties (long circulating times), and inability to penetrate deep into tissue (due to the large size of ~150 kDa) (3). Therefore, investigators are constantly developing and evaluating new alternatives to the Ab-based imaging agents (3).

Recently, a small (~7 kDa) Z_HER2:342_ affibody was engineered (4) and labeled with radionuclides such as ^99m^Tc or ^111^In for the detection of HER2-overexpressing tumors with the use of SPECT (2). Later, the affibody and several of its structural derivatives were labeled with ^99m^Tc and used to detect HER2-expressing cancers under preclinical and clinical conditions (for details on the structural derivatives, see Ekblad et al.) (5, 6). It has been shown that a hexa-histidine tag (H_6_; also facilitates purification of the H_6_-bearing compound by immobilized metal ion affinity chromatography) bearing dimeric Z_HER2:342_ could be labeled with ^99m^Tc-tricarbonyl ([^99m^Tc(CO)_3_]^+^) to obtain [^99m^Tc(CO)_3_]^+^-H_6_-(Z_HER2:342_)_2_, and that the radiochemical was suitable to visualize the expression of HER2 in tumor-bearing mice (7). However, for the duration of the study, a higher amount of radioactivity was observed to accumulate in the liver compared to the tumors. From these observations the investigators concluded that, because the liver is often the organ to which a cancer metastasizes, H_6_-(Z_HER2:342_)_2_ was suitable only for the imaging of extrahepatic tumors. Other investigators have also shown that an H_6_ tag located on the N-terminal on a ^99m^Tc-labeled anti-HER2 affibody leads to increased accumulation of label in the hepatic tissue (8, 9). On the basis of a hypothesis that the uptake of the labeled compound by the liver could be reduced by moving the H_6_ tag from the N-terminal of the Z_HER2:342_ affibody or by increasing the hydrophilicity of the tag, two new tracers were constructed by Tolmachev et al. (10). In one construct, the H_6_ tag was moved from the N-terminal of the affibody to the C-terminal to obtain Z_HER2:342_-H_6_; in the second construct, the tag located on the N-terminal of the affibody was made more hydrophilic by alternating glutamatic acid residues with the histidines to generate HEHEHE ((HE)_3_) and obtain (HE)_3_-Z_HER2:342_. These constructs were subsequently labeled with [^99m^Tc(CO)_3_]^+^ to form [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, respectively. The biodistribution patterns of these radiolabeled affibodies were respectively studied in normal and LS174T (a human colon cancer cell line that has a low expression of HER2) xenograft tumor-bearing nude mice and compared to that of the parent affibody, Z_HER2:342_ (described previously in (11)), which had an H_6_ tag on the N-terminal and was labeled with [^99m^Tc(CO)_3_]^+^ ([^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_). This chapter describes the results obtained with [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ and are compared to those obtained with [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_. Results obtained with [^99m^Tc(CO)_3_]^+^-H_6_ -Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ are described in separate chapters of MICAD (www.micad.nih.gov) (12, 13).

### Other Sources of Information

Affibody Z_HER2:342_ chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ZHER2+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man).

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein).

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR.

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%28CO%293%5D-H6-ZHER2%3A342&cmd=DetailsSearch)]

The production and purification of H_6_-ZHER_2:342_, Z_HER2:342_-H_6_, and (HE)_3_-Z_HER2:342_ were performed as described by Tolmachev et al. (10). The purity of the two hexa-histidine- and the (HE)_3_-linked affibodies was reported to be 98%. The molecular weights of H_6_-Z_HER2:342_, Z_HER2:342_-H_6_, and (HE)_3_- Z_HER2:342_ were reported to be 8.2 kDa, 7.873 kDa, and 7.836 kDa, respectively. Labeling of the tagged affibodies with [^99m^Tc(CO)_3_]^+^ was also described by Tolmachev et al. (10). The radiochemical yield and purity of the three tracers were 80% and >95%, respectively. The specific activities of the three labeled affibodies were 14–15.8 GBq/μmol (378–426 mCi/μmol). Radio-colloid formation in the final preparation of each radiolabeled affibody was <1.5% as determined with reversed-phase high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

[^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were reported to be stable in phosphate-buffered saline for at least 24 h at room temperature (23°C). At the end of incubation, 98.5 ± 0.8%, 97.2 ± 0.2%, and 96.7 ± 0.0% of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively, were reported to be intact as determined with instant thin-layer chromatography (10). A challenge with 500- or 1,000-fold excess histidine at 37°C for 1 h showed that >98% of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ and >95% of [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ was intact at the end of the incubation period. The association equilibrium constant (KD), the association rate constant (Ka), and the dissociation rate constant (Kd) for [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ were 18 pM, 7.0 × 10^6^ M^-1^s^-1^, and 1.2 × 10^-4^ s^-1^, respectively, as determined with biosensor analysis.

Using SKOV-3 (an ovarian cancer cell line with high expression of HER2), DU-145 (a prostate cancer cell line that has a low expression of HER2), and PC-3 (another prostate cancer cell line that has a low expression of HER2) cells, the receptor-binding specificity values of the labeled affibodies were reported to be 48.0 ± 2.0, 3.19 ± 0.04, and 3.0 ± 0.2, respectively, for [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_; 48.9 ± 0.8%, 6.1 ± 0.2%, and 6.7 ± 0.1%, respectively, for [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_; and 46.0 ± 2.0%, 9.0 ± 0.4%, and 6.8 ± 1.0%, respectively, for [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ (10). Pretreatment of the cells with 1,000-fold excess unlabeled H_6_-Z_HER2:342_ reduced the receptor binding on the SKOV-3, DU-145, and PC-3 cells significantly (P < 0.0005) to 0.9 ± 0%, 1.4 ± 0.3%, and 0.8 ± 0.1%, respectively, for [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_; to 2.3 ± 0.5%, 3.0 ± 0.3%, and 3.6 ± 0.1%, respectively, for [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_; and 3.0 ± 0.1%, 3.1 ± 0.2%, and 3.4 ± 0.2%, respectively, for [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_. Cellular internalization of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ by the SKOV-3 cells after 24 h incubation at 37°C was determined to be 65.3 ± 1.1%, 80.1 ± 0.5%, and 47.7 ± 0.1%, respectively. The antigen binding capacity of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ in the presence of 100-fold excess receptor concentration (using intact SKOV-3 cells) was reported to be 70.3 ± 7.3%, 79.6 ± 0.6%, and 80.5 ± 0.4%, respectively. Similar antigen binding specificities have been reported by other investigators for ^99m^Tc-labeled affibodies (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20rodentia&cmd=DetailsSearch)]

The biodistribution patterns of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were studied in normal male Naval Medical Research Institute (NMRI) mice (n = 4 animals/time point) after intravenous injection of the respective tracers as described by Tolmachev et al. (10). Accumulated radioactivity in various organs of the animals was determined at 4 h and 24 h postinjection (p.i.) and was presented as percent of injected dose per gram tissue (% ID/g). In the blood, the radioactivity levels from [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were 0.28 ± 0.04% ID/g, 0.19 ± 0.06% ID/g, and 0.9 ± 0.4% ID/g, respectively, at 4 h p.i.; this decreased to 0.10 ± 0.02% ID/g, 0.07 ± 0.02% ID/g, and 0.19 ± 0.04% ID/g, respectively, by 24 h p.i. At 4 h p.i., the kidneys had uptake values of 80.0 ± 4.0% ID/g, 92.0 ± 23.0% ID/g, and 100.0 ± 16.0% ID/g radioactivity from [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively. By 24 h p.i., the kidney uptake values had decreased to 43.0 ± 6.0% ID/g, 45.0 ± 6.0% ID/g, and 56.0 ± 10.0%, respectively. In the liver, the accumulations of the label from [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ at 4 h p.i. was 0.9 ± 0.2% ID/g, 10.0 ± 3.0% ID/g, and 5.0 ± 1.0% ID/g, respectively; by 24 h p.i., the tracer levels decreased to 0.61 ± 0.08% ID/g, 7.0 ± 1.0% ID/g, and 2.9 ± 0.5% ID/g, respectively. The reduced accumulation of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ in the liver was attributed to the lower hydrophobicity at the N-terminal of the affibody due to the presence of the (HE)_3_ tag (1). At 4 h p.i., the uptake values in the spleen were 0.17 ± 0.03% ID/g, 1.3 ± 0.3% ID/g, and 0.8 ± 0.1% ID/g with [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, respectively; by 24 h p.i., the accumulation in this organ decreased to 0.10 ± 0.02% ID/g, 0.8 ± 0.1% ID/g, and 0.47 ± 0.07% ID/g, respectively. All other organs showed uptake of <1.0% ID/g radioactivity from the three tracers at both time points. These observations indicated that radioactivity from the three labeled affibodies was rapidly cleared from the blood and was excreted primarily through the kidneys. The study also showed that, compared to [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, approximately 2-fold and 10-fold less radioactivity accumulated in the liver with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, respectively; however, clearance of the latter labels from the blood was slower than the former (10). No in vivo blocking studies were reported with any of the radiolabeled affibodies.

In another study, the biodistribution patterns of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, and [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ were investigated in NMRI nude mice (n = 4 animals/group) bearing LS174T cell xenograft tumors (10). The uptake values of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ in the kidneys, liver, and the xenograft tumors at 4 h p.i. were 70.0 ± 10.0% ID/g, 0.88 ± 0.05% ID/g, and 2.6 ± 0.4% ID/g, respectively, and the T/B, T/L, T/K, and T/M ratios were 81.0 ± 2.0, 3.0 ± 0.5, 0.038 ± 0.009, and 40.0 ± 3.0, respectively. At 4 h p.i., the accumulations of radioactivity from [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ in the kidneys, liver, and the xenograft tumors were 82.0 ± 9.0% ID/g, 8.1 ± 0.8% ID/g, and 2.2 ± 0.3% ID/g, respectively. The tumor/blood (T/B), tumor/liver (T/L), tumor/kidney (T/K), and the tumor/muscle (T/M) ratios with this tracer were 4.5 ± 0.1, 0.29 ± 0.04, 0.028 ± 0.002, and 21.0 ± 0.2, respectively. For [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_, the label uptake values in the kidneys, liver, and the xenograft tumors were 67.0 ± 13.0% ID/g, 4.3 ± 0.8% ID/g, and 3.2 ± 0.9% ID/g, respectively, and the T/B, T/L, T/K, and T/M ratios were 3.0 ± 0.4, 0.7 ± 0.1, 0.047 ± 0.006, and 17.0 ± 3.0, respectively. This showed that, compared to [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_, there was higher tumor uptake of [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, and the highest uptake was with the (HE)_3_ affibody. In addition, among the three labeled affibodies, [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ had the lowest uptake in the liver. This indicated that changing the location of the H_6_ tag from the N-terminal to the C-terminal or making the N-terminal tag of the affibody more hydrophilic reduced the uptake of radioactivity in the liver and other tissues but increased accumulation of the label in the HER2-positive tumors. No blocking studies with either tracer using the tumor-bearing mice were reported.

Gamma planar imaging of a tumor-bearing mouse showed that the uptake patterns of [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ and [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ in the animals were similar to those observed during the biodistribution studies (10). However, it was clear from the images that the accumulation of radioactivity in the tumors was higher with [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ than with [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_. No imaging studies were reported with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available

## References

1 Tolmachev V., Rosik D., Wallberg H., Sjoberg A., Sandstrom M., Hansson M., Wennborg A., Orlova A. (2010). Imaging of EGFR expression in murine xenografts using site-specifically labelled anti-EGFR 111In-DOTA-Z EGFR:2377 Affibody molecule: aspect of the injected tracer amount. Eur J Nucl Med Mol Imaging.
2 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
3 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
4 Wahlberg E., Lendel C., Helgstrand M., Allard P., Dincbas-Renqvist V., Hedqvist A., Berglund H., Nygren P.A., Hard T. (2003). An affibody in complex with a target protein: structure and coupled folding. Proc Natl Acad Sci U S A.
5 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
6 Ekblad T., Orlova A., Feldwisch J., Wennborg A., Karlstrom A.E., Tolmachev V. (2009). Positioning of 99mTc-chelators influences radiolabeling, stability and biodistribution of Affibody molecules. Bioorg Med Chem Lett.
7 Orlova A., Nilsson F.Y., Wikman M., Widstrom C., Stahl S., Carlsson J., Tolmachev V. (2006). Comparative in vivo evaluation of technetium and iodine labels on an anti-HER2 affibody for single-photon imaging of HER2 expression in tumors. J Nucl Med.
8 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.
9 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.
10 Tolmachev V., Hofstrom C., Malmberg J., Ahlgren S., Hosseinimehr S.J., Sandstrom M., Abrahmsen L., Orlova A., Graslund T. (2010). HEHEHE-tagged affibody molecule may be purified by IMAC, is conveniently labeled with [(m)Tc(CO)](+), and shows improved biodistribution with reduced hepatic radioactivity accumulation. Bioconjug Chem.
11 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
12 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the N-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the C-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.